# N,N´-Bis(2,3-dihydroxypropyl)-5-[N-(2-hydroxyethyl)-glycolamidol]-2,4,6-triiodoisophthalamide

Chemical name: | N,N´-Bis(2,3-dihydroxypropyl)-5-[N-(2-hydroxyethyl)-glycolamidol]-2,4,6-triiodoisophthalamide
Abbreviated name: | Ioversol
Synonym: | Optiray^®^ ,MP-328
Agent Category: | Compound
Target: | Non-targeted, blood pool, extracelluar space
Target Category: | Nonspecific filling of blood vessels and tissues
Method of detection: | X-ray, CT
Source of signal/ contrast: | Iodine (I)
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Ioversol%20OR%20optiray)]

N,N´-bis(2,3-dihydroxypropy)-5-[N-(2-hydroxyethyl)-glycolamidol]-2,4,6-triiodoisophthalamide (ioversol) is a nonionic X-ray contrast agent used to aid the radiographic visualization of blood vessels, heart, head, and body (1). Ioversol is approved by the United States Food and Drug Administration for contrast enhancement in peripheral and coronary arteriography and left ventriculography and for computed tomographic (CT) imaging of the head and body (2).

X-Ray imaging (planar and tomographic) techniques depend on tissue density differences which provide the image contrast produced by X-ray attenuation between the area of interest and surrounding tissues (3, 4). Contrast enhancement (opacification) with use of contrast agents increases the degree of contrast and improves the differentiation of pathological processes from normal tissues. Because iodine, an element of high atomic density, casuses high attenuation of X-rays within the diagnostic energy spectrum, water-soluble and reasonably safe iodinated contrast agents in intravenous injectable forms have been developed for clinical applications (5, 6).

Water-soluble, intravenous X-ray contrast agents are generally organic iodine compounds that contain one or more tri-iodinated benzene rings (7, 8). When injected intravenously, they are largely distributed in the extracellular fluid space and excreted unchanged by the kidneys (9). Contrast enhancement of a region of interest depends on the route of administration, delivery of the agent to the area by blood flow, and the final iodine concentration in the region. There are two basic types of these compounds: ionic and nonionic agents. The first monomeric ionic compound in the form of the 2,4,6-triiodobenzene acetrizoic acid, was synthesized by Wallingford (5). Most ionic contrast agents are derived from the basic structures of 3,5-diamino-2,4,6-triiodobenzoic acid, 5-amino-2,4,5-triiodoisophthalic acid, or 2,4,6-tri-iodobenzene-1,3,5-tricarbonic acid. In addition to developing monoacidic ionic dimers, nonionic compounds have also been developed to improve the tolerability of these agents in patients. The basic strategy of developing nonionic agents is to eliminate the electrical charges in the structure, which will lead to a reduction in osmolality of the compound. Because osmolality is related to the number of particles in solution, the challenge is to reduce the number of particles and maintain the iodine concentration (10). This was generally achieved by conversion of the carboxyl groups to hydroxyalkylamide groups (11). Further improvement was made by replacing the amino sugar with aminoalcohols to produce heat-stable hydroxyalkylamides to allow product sterilization (12).

Ioversol is a monomeric nonionic, tri-iodinated contrast agent that is characterized by relatively high hydrophilicity (13). Bonnemain et al. (14) discussed the concept of evenly distributed facial hydrophilicity, which led to the high hydrophilicity (log P octanol/water = -2.98) of ioversol. The current commercial formulations (http://www.imaging.mallinckrodt.com/Products/Product.asp?ProductID=81) contain iodine concentrations of 160, 240, 300, 320 and 350 mg of iodine/ml (mg I/ml) with corresponding osmolality values (mOsm/g water) of 355, 502, 651, 702, and 792, respectively (2). The corresponding viscosity values (cps at 37 ºC) are 1.9, 3.0, 5.5, 5.8, and 9.0, respectively.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioversol%20OR%20optiray%29%20AND%20synthesis)]

The synthesis steps involved in the production of X-ray contrast agents are well established organic reactions (7). Hoey et al. (15) described the basic approach of synthesizing derivatives of isophthalamic acid as contrast agents. The synthesis of ioversol involved an S_N_2 reaction in which the amine was a nucleophile and an alkyl halide was the substrate. The reaction was carried out at a basic pH to avoid deactivation of the amino group. Lin (16) first described the synthesis that involved the synthesis of N,N´-bis(2,3-dihydroxypropyl)-5-glycolamido-2,4,6-triiodoisophthalamide from the starting chemical of 5-amino-2,4,6-triiodoisophthalic acid. This compound was then reacted with chloroethanol for 3 days, and 1 N NaOH and 2-chloroethanol were added and reacted for 3 more days. Additional portions of 1 N NaOH and 2-chloroethanol were added and reacted overnight. After trituration with methanol, filtration, and purification by preparative liquid chromatography, the final yield was 47.7%. Bailey et al. (17) reported a synthesis in which they added 2-bromoethylacetate and potassium carbonate to a solution of 5-acetoxyacetamido-N,N´-bis(2,3-diacetoxypropyl)2,4,6-triiodoisophthalamide in dimethylsulfoxide. The mixture was stirred until the reaction was complete. The resulting compound was then hydrolyzed with water containing sulfuric acid to produce ioversol. Ioversol prepared by this method required extensive purification to remove impurities. Bosworth et al. (18) reported a high-efficiency reverse osmosis method to remove the low- molecular impurities. Bailey et al. (17) described an additional step involving a selective hydrolysis reaction so that most of the unwanted impurities were reduced and/or eliminated

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioversol%20OR%20optiray%29%20AND%20%28%22in%20vitro%22%29)]

Ralston et al. (1) reported the genetic toxicology of ioversol (32% iodine w/v) ioversol in several in vitro systems. The mutagenicity of ioversol was evaluated in the in vitro microbial reverse mutation assay, mammalian forward mutation assay, and mammalian chromosomal aberration assay. Ioversol was not considered to be mutagenic in any of the three assays.

Heinrich et al. (19) studied the cytotoxic effects of iodinated contrast agents on renal tubular LLC-PK1 cells (porcine origin) in vitro. Ioversol in concentrations of 49.25 and 98.5 mM were studied. An ionic agent (ioxithalamate) showed a stronger cytotoxic effect than that of ioversol with cell viability of 4 ± 0.3% and 32± 2%, respectively. The study suggested that both hyperosmolality and direct cytotoxic effects contributed to the overall cytotoxic effects. Oldroyd et al. (20) used the isolated perfused rat kidney model to showed that ioversol (20 mg I/ml) produced endothelin-mediated effects on renal hemodynamics. Krause et al. (21) found that ioversol (n-butanol/water partition coefficient = 0.038) had in vitro effects similar to those of iopamidol (nonionic agent with n-butanol/water partition coefficient = 0.100) on rabbit erythrocyte morphology, lysozyme inhibition, and coagulation time. In a study involving cultured bovine aorta endothelial cells (ECs) and smooth muscle cells (SMCs), Sawmiller et al. (22) found that ECs were more severely affected by iothalamate (ionic agent), but that SMCs were more severely affected by Ioversol and iopamidol (nonionic agents).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioversol%20OR%20optiray%29%20AND%20rodentia)]

Ralston et al. (1) examined the reproductive, developmental, and genetic toxicology of ioversol in mice and rats. No teratogenic, fertility, or reproductive effects were observed in rats receiving intravenous doses up to 3.2 g of I(iodine)/kg/day. Offspring of dams treated with ioversol developed and reproduced in a normal fashion. A mammalian micronucleus assay was performed in mice that had received single intravenous doses up to 3.2 g I/kg, and it showed that ioversol did not induce a significant increase in micronuclei in mouse bone marrow. In another study (10), the medium lethal dose (LD_50_) for the acute intravenous toxicity of ioversol (32% iodine (I) w/v) in mice and rats was 17 and 15 g I/kg, respectively. The LD_50_ for acute intracisternal toxicity (43% I w/v) in rats was 1,000 mg of iodine/kg for females and > 1,200 mg I/kg for males. A study of the subacute intravenous toxicity (32% I w/v) in rats that received daily injections for 4 weeks showed that only significant effect was slight-to-moderate renal tubular cytoplasmic vacuolation at doses of 0.8 and 3.2 g I/kg/day dose levels. Ralston et al. (23) studied the effect of intracarotid injection in rats. Bilateral intracarotid injection of ioversol produced slight but transient changes in heart rate, respiratory rate, and mean arterial pressures. No arrhythmias, respiratory arrests, or alteration in the blood-brain barrier (BBB) were observed.

Wible et al. (24) studied the neurotoxicity of ioversol and other contrast agents after intracisternal administration of doses up to 1000 mg I/kg in rats. Signs of toxicity included tremors, head shaking and vocalization, convulsions, chewing and hypoactivity, and apnea. After performing a comparison with other less-hydrophilic nonionic agents (iopromide, iohexol, and iopamidol), the authors suggested that agents with higher hydrophilicity might produce lesser central nervous sytem toxicity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28ioversol%20OR%20optiray%29%20AND%20%28dogs%20OR%20pigs%20OR%20rabbits%20OR%20sheeps)]

Ralston et al. (1) assessed the effects of ioversol on the pregnancy and development in rabbits. Treatment with doses of 0.2, 0.8, and 3.2 g I/kg/day from day 6 to day 18 of pregnancy did not adversely affect the incidence of malformations, skeletal and visceral anomalies, or skeletal variants. In another study (10), the acute intravenous toxicity (LD_50_) values of ioversol (32% I w/v) for rabbits and dogs were ≥25 and >12 g I/kg, respectively. In a study of acute intrathecal toxicity in dogs showed that signs of toxicity were limited to prolonged lethargy within the first few hours after injection of 240 mg I/kg. Ralston et al. (23) studied the intravenous pharmacokinetics in dogs. They reported that regardless of the route of injection, they observed only minimal effects on the heart rate and minimal to moderate decreases in myocardial contractility, left ventricular pressure, mean arterial pressure, pulmonary vascular resistance, and systemic vascular resistance.

Coveney and Robbins (25) used ^125^I-labeled ioversol to study the biodistribution and excretion of ioversol (0.2 g I/kg and 1 g I /kg) in dogs. Biexponential blood clearance was observed in 3 of 4 dogs. Average distribution t_½_s were 2.5 to 3.5 min, and elimination t_½_s were 51 to 54 min. Volumes of distribution were 25-27% of the body weight which was consistent with extracellular fluid space distribution. Ioversol appeared to be excreted unchanged by the kidneys with ~40% of injected dose recovered in the urine at 2 h after injection. Very little of the radioactivity was found in tissues assayed at 48 h.

Evill et al. (26) studied the chemotoxic effects of ioversol (320 mg I/ml) and other contrast agents in rabbits with use of ^99m^Tc pertechnetate to measure BBB injury. The ^99m^Tc uptake (BBB injury) was calculated based on the difference in the blood/brain activity ratio (radioactivity in µg of blood per g of brain) between a BBB region that was exposed to the agent and a control BBB region (no exposure). For ioversol, this ratio was 6.06. In comparison, the values for mannitol (control), iohexol, iodixanol, and iotrolan were 0.15, 12.11, 9.46, and 4.21, respectively.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioversol%20OR%20optiray%29%20AND%20%28primate%20NOT%20human%29)]

Ralston et al. (10) studied the acute neurotoxicity of ioversol (27% I w/v) in cynomolgus monkeys. After lumbar intrathecal injection of ioversol (60 mg of iodine/kg of body weight), transient tremors and muscular fasciculations were observed immediately, but the symptoms were absent at 1 h. No histologic abnormalities were found on the spinal leptomeninges at 12 weeks after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioversol%20OR%20optiray%29%20AND%20humans)]

Wilkins et al. (27) conducted a single-blind randomized study of the safety and pharmacokinetics of ioversol (320 mg of iodine/ml in doses of 50, 100, and 150 ml) in 24 healthy volunteers. No significant changes were observed in physical examination, vital signs, electrocardiography, and biochemical and hematological data. Biphasic blood clearance (n = 6) was observed with t_½_α (min) and t_½_β (h) determined to be 15.5 ± 3.5 and 2.06 ± 0.13 for the 50 ml dose. For the 150-ml dose, t_½_α and t_½_β were 18.9 ± 3.2 min and 2.04 ± 0.04 h, respectively. The urinary excretion t_½_β for the 50-ml and 150-ml doses were 1.88 ± 0.14 h and 1.73 ± 0.25 h, respectively. The volumes of distribution (ml/kg), V_dβ_ and V_dss_, for the 50-ml dose were 394 ± 22 and 353 ± 12, respectively. For the 150-ml dose, the values were 410 ± 25 and 360 ± 19 ml/kg, respectively.

McClennan (28) and Benamor et al. (29) reported on the clinical safety of ioversol based on 23 double-blind, controlled, parallel group studies and 9 open-label studies. A total of 1,186 patients participated in the trials and received a mean contrast dose of 1.6 ml/kg (ioversol, 320 mg I/ml and 240 mg I/ml for venography only), or a mean iodine dose of 470.7 mg/kg. About 91% of patients reported no or mild pain associated with the injection. Whereas about 5.8% of patients had one or more adverse reactions. Nausea (1.0%), headache (0.8%), vomiting (0.5%), blurred vision (0.4%), vertigo (0.4%), and lightheadedness (0.3%) were the most common reactions. In comparison, the reference group that received ionic contrast agents reported an adverse reaction rate of 14.8%. No significant changes of renal function up to 96 h after injection were observed. The diagnostic efficacy of ioversol appeared to be comparable to the efficacies of both ionic and nonionic agents with respect to diagnostic quality. Le Mignon et al. (13) reported the European clinical experience of 472 patients who received ioversol (300 mg I/ml or 350 mg I/ml). About 11% of patients had adverse reactions, and Ioversol was found to be 99% useful in all radiologic applications. In 76% of the cases, image quality was judged to be good or excellent. In 1996, Floriani et al. (30) performed a metaanalysis of data from all available randomized, double-blind trials of ioversol. A total of 1931 patients were included in the analysis which indicated that ioversol was considered diagnostic in 99.3% of examinations, with good to excellent enhancement quality in 89.3% of cases.

Other studies have indicated that ioversol appears to have safety, tolerability, and efficacy profiles comparable to other nonionic contrast agents in various radiographic studies of the brain, heart, blood vessels, kidneys, and whole body [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Ioversol%20OR%20optiray%29%20AND%20%28blood%20vessels%20OR%20brain%20OR%20heart%20OR%20kidney%20OR%20whole%20body%29)].

## Supplemental Information

[Disclaimers]

Ioversol Package Insert

Ioversol Bulk Pack Package Insert

Ioversol Material Safety Data Sheet

## References

1 Ralston W.H., Robbins M.S., James P. (1989). Reproductive, developmental, and genetic toxicology of ioversol. Invest Radiol.
2. Optiray 350, Optiray 320, Optiray 300, Optiray 240, Optiray 160, in Optiray package insert. 2000, Mallinkcrodt, INc.: St. Louis. p. 1-2.
3. Swanson, D.P. and M.B. Alpern, Contrast media for computed tomography: Intravascular, intracavitary, xenon, reticuloendothelial, in Pharmaceuticals in medical imaging, D.P. Swanson, H. M. Chilton and J. H. Thrall, Editor. 1990, Macmillan Publishing Company: New York. p. 99-124.
4. Hoey, G.B. and K.R. Smith, Chemistry of X-ray contras media, in Radiocontrast agents, M. Sovak, Editor. 1984, Springer-Verlag: New York. p. 23-125.
5 Wallingford V.H. (1953). The development of organic iodine compounds as x-ray contrast media. J Am Pharm Assoc Am Pharm Assoc (Baltim).
6 Sovak M., Ranganathan R., Lang J.H., Lasser E.C. (1977). and Concepts in design of improved intravascular contrast agents. European Society of cardiovascular Radiology, Uppsala, (May): p. 25-27.
7. Gries, H., Chemistry of X-ray contrast agents, in Textbook of contrast media, P. Dawson, D.O. Cosgrove, and R.G. Grainger, Editors. 1999, Isis Medical Media Ltd.: Oxford. p. 15-22.
8 Almen T. (1969). Contrast agent design. Some aspects on the synthesis of water soluble contrast agents of low osmolality. J Theor Biol.
9. Dawson, P., Pharmacokinetics of water-soluble iodinated X-ray contrast agents, in Textbook of contrast media, P. Dawson, D.O. Cosgrove, and R.G. Grainger, Editors. 1999, Isis Medical Media Oxford. p. 61-74.
10 Ralston W.H., Robbins M.S., Coveney J., Blair M. (1989). Acute and subacute toxicity studies of ioversol in experimental animals. Invest Radiol.
11 Almen T. Development of nonionic contrast media Invest Radiol 1985 20Suppl1 S2 9 2579043
12 Sovak M. Ranganathan R. Stability of nonionic water-soluble contrast media: implications for their design Invest Radiol 1980 15Suppl6 S323 8 7203944
13 Le Mignon M.M., Azau C., Arthaud A., Bonnemain B. (1991). Preliminary European intravenous clinical experience with a new, low osmolar, nonionic contrast medium: ioversol (Optiray). Eur J Radiol.
14 Bonnemain B., Meyer D., Schaefer M., Dugast-Zrihen M., Legreneur S., Doucet D. (1990). New iodinated, low-osmolar contrast media. A revised concept of hydrophilicity. Invest Radiol.
15 Hoey G.B., Rands R.D., Delamater G., Chapman D.W., Wiegert P.E. (1963). Synthesis of Derivatives of Isophthalamic Acid as X-Ray Contrast Agents. J Med Chem.
16 Lin Y. (1982).
17. Bailey, A.R., S.S. Sathe, A.T. Spears, R.C. Wisneski, and K.M. T., Improved Synthesis of Ioversol, in International search report, W.I.P. Organization, Editor. 1993, Mallinckrodt Medical, Inc. p. 1-11.
18. Bosworth, M.E., T.J. Dunn, Hall, W. E., R.G. Johnson, M.T. Kneller, Y. Lin, R.A. Wallace, D.H. White, and D.M. Wong, Purification of crude ioversol using reverse osmosis, U.S.P. Office, Editor. 1992, Mallinckrodt Medical Inc.: United States. p. 1-8.
19 Heinrich M.C., Kuhlmann M.K., Grgic A., Heckmann M., Kramann B., Uder M. (2005). Cytotoxic effects of ionic high-osmolar, nonionic monomeric, and nonionic iso-osmolar dimeric iodinated contrast media on renal tubular cells in vitro. Radiology.
20 Oldroyd S.D., Haylor J.L., Morcos S.K. (1995). The acute effect of ioversol on kidney function: role of endothelin. Eur J Radiol.
21 Krause W., Miyazawa T., Uchimoto R., Murayama C., Fritz-Zieroth B., Press W.R., Frenzel T. (1995). Comparison of iopamidol and ioversol in vitro and in animal studies. Arzneimittelforschung.
22 Sawmiller C.J., Powell R.J., Quader M., Dudrick S.J., Sumpio B.E. (1998). The differential effect of contrast agents on endothelial cell and smooth muscle cell growth in vitro. J Vasc Surg.
23 Ralston W.H., Robbins M.S., Coveney J.R. (1989). Hemodynamic effects of ioversol in the dog and rat. Invest Radiol.
24 Wible J.H., Barco S.J., Scherrer D.E., Wojdyla J.K., Adams M.D. (1995). Neurotoxicity of non-ionic X-ray contrast media after intracisternal administration in rats. Eur J Radiol.
25 Coveney J.R., Robbins M.S. (1989). Biodistribution and excretion of 125I ioversol in conscious dogs. Invest Radiol.
26 Evill C.A., Wilson A.J., Sage M.R. (1990). Chemotoxic effects of low-osmolar contrast media on the blood-brain barrier. Invest Radiol.
27 Wilkins R.A., Whittington J.R., Brigden G.S., Lahiri A., Heber M.E., Hughes L.O. (1989). Safety and pharmacokinetics of ioversol in healthy volunteers. Invest Radiol.
28 McClennan B.L. (1989). Clinical summary of initial intravenous administration of ioversol. Invest Radiol.
29 Benamor M., Aten E.M., McElvany K.D., Lankin D.G., James M.A., Buy-Gandal T., Harashe L.T., Weinandt W.J. (1989). Ioversol clinical safety summary. Invest Radiol.
30 Floriani I., Ciceri M., Torri V., Tinazzi A., Jahn H., Noseda A. (1996). Clinical profile of ioversol. A metaanalysis of 57 randomized, double-blind clinical trials. Invest Radiol.